# Microbubbles-echistatin

Chemical name: | Microbubbles-echistatin
Abbreviated name: | MB_E_
Synonym:
Agent category: | Polypeptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Ultrasound
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=914065), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_003183.4) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=6868) for more information about echistatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20echistatin)]

Ultrasound is the most widely used imaging modality (1) and is expanding its role in noninvasive molecular imaging with ligand-carrying microbubbles (2). Microbubbles are comprised of spherical cavities filled by a gas encapsulated in a shell. The shells are made of phospholipids, surfactant, denatured human serum albumin or synthetic polymer. Ligands and antibodies can be incorporated into the shell surface of microbubbles. Microbubbles are usually 2 to 8 μm in size. They provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (3-5). They are also potentially used for drug and gene delivery (6).

Angiogenesis is the formation of new blood capillaries and vessels from existing vessels (7-9). It involves the degradation of the basal membrane surrounding the parental vasculature, and the proliferation of endothelial and smooth muscle cells to form new vessels, resulting in an improvement in tissue perfusion and function. The major stimuli for angiogenesis include ischemia, hypoxia, inflammation, and shear stress (10). A large number of endogenous angiogenic factors are involved in angiogenesis (11), including vascular endothelial growth factor (VEGF), basic fibroblast growth factor (bFGF), interleukin-8 (IL-8), and transforming growth factor (TGF-β). Extracellular matrix and proteolytic enzymes as well as integrins are also involved during angiogenesis (12). There are also endogenous inhibitors of angiogenesis such as, angiostatin, endostatin and platelet factor-4 (13, 14).

Tumor angiogenesis represents a continuous and important process in tumor development in which the tumor attempts to gain an independent blood supply (15). This process is driven by the tumor's chronic overproduction of pro-angiogenic factors, which bind to receptors on nearby vessel endothelial cells. Angiogenesis is essential for the growth of solid tumors and their metastases. Imaging angiogenesis may be useful for monitoring angiogenic treatments of tumors and cardiovascular diseases (9, 16, 17). The α_v_β_3_ integrin is strongly expressed on tumor cells and activated endothelial cells. In contrast, expression of α_v_β_3_ integrin is weak on resting endothelial cells and most normal tissues. A tripeptide sequence consisting of Arg-Gly-Asp (RGD) is identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins including α_v_β_3_.

Echistatin is a 5.4 kDa snake venom disintegrin that binds to α_v_β_3_ integrin with high affinity (18). Microbubbles were targeted by conjugation of echistatin to the shell surface and used to image angiogenesis with contrast-enhanced ultrasound (CEU) (19). Microbubbles-echistatin may provide a noninvasive method for assessing therapeutic angiogenesis (20).

### Related Resource Links:

- Chapters in MICAD (Echistatin (http://www.ncbi.nlm.nih.gov/books?term=Echistatin%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Echistatin (http://www.ncbi.nlm.nih.gov/gene/6868))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Echistatin (http://www.ncbi.nlm.nih.gov/omim/603710))
- Clinical trials (Echistatin (http://www.clinicaltrials.gov/ct2/results?term=disintegrin))
- Drug information in FDA (Echistatin (http://google2.fda.gov/search?q=endostatin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=0&y=0))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20echistatin)]

For targeted microbubbles, biotinylated microbubbles were first prepared by sonication of an aqueous dispersion of decafluorobutane gas, distearoylphosphatidylcholine, polyethyleneglycol-(PEG-) stearate, and distearoylphosphatidylethanolamine-PEG-biotin. Microbubbles were combined with streptavidin, washed, and combined with biotinylated echistatin (MB_E_) or monoclonal antibody (mAb R3-34) against α_v_ integrin (MB_α_). Control lipid microbubbles (MB_C_) were also prepared. For confocal microscopy, microbubbles were fluorescently labeled by dioctadecyl tetramethylindocarbocyanine or dioctadecyl oxacarbocyanine. For perfusion imaging, nontargeted lipid-shelled microbubbles (MP1950) were also prepared. Microbubble concentration and size distribution were determined by electrozone sensing. The microbubbles are about 2-4 microns in diameter. A ligand to microbubble ratio was estimated to be about 60,000 by flow cytometry (19-21).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20echistatin)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20echistatin%20and%20rodentia)]

The effect of bFGF on angiogenesis was assessed with microbubbles targeted to α_v_β_3_ integrin_._ FGF-2 pellets or control pellets were implanted intrascrotally in mice for 4 days (19). FGF-2 stimulation of cremaster microvessel formation was confirmed by fluorescent and intravital microscopy as compared to control mice. Microvascular retention was significantly greater for MB_E_ and MB_α_ than that for MB_c_. Retained MB_E_ and MB_α_ attached directly to the microvascular endothelial surface. Microbubble retention in control mice was minimal. Matrigel plugs enriched with FGF-2 were subcutaneously implanted in mice for 10 days. Neovessels within the matrigel were positive for α_v_-integrins by immunostaining. CEU showed significantly greater acoustic intensity for MB_E_ (16.0±5.9 U) and MB_α_ (17.0±5.5 U) compared with MB_c_ (5.8±2.6 U). The signal from targeted microbubbles (MB_E_ and MB_α_) correlated well (r=0.90) with the matrigel blood volume determined by CEU perfusion imaging. CEU with microbubbles targeted for α_v_-integrins may provide a noninvasive method for assessing therapeutic angiogenesis.

Malignant gliomas were produced in 14 athymic rats by intracerebral implantation of U87MG human glioma cells (20). On day 14 or day 28 after implantation, CEU was performed with MB_E_ and MB_c_. CEU perfusion imaging with MB_c_ was used to derive tumor microvascular blood volume and blood velocity. Vascular α_v_-integrin was expressed on the microvascular endothelial cells of tumor neovessels as assessed by immunohistochemistry. Tumor size increased significantly from 14 to 28 days (2±1 versus 35±14 mm^2^). Tumor blood volume increased by about 35% from day 14 to day 28, whereas microvascular blood velocity decreased, especially at the central portions of the tumors. On confocal microscopy, MB_E_ (7 to 20 per 10 optical fields) but not MB_c_ (<1 per 10 optical fields) were retained preferentially within the tumor microcirculation. CEU signal from MB_E_ in tumors increased significantly from 14 to 28 days (1.7±0.4 versus 3.3±1.0 relative units). CEU signal from control microbubbles increased non-significantly from 1.1±0.2 to 1.2±0.3 relative units from 14 days to 28 days. CEU signal from MB_E_ was greatest at the periphery of tumors, where α_v_β_3_ -integrin expression was most prominent, and correlated well with tumor microvascular blood volume (r=0.86). CEU with MB_E_ can non-invasively detect early tumor angiogenesis. This technique, in conjunction with changes in blood volume and velocity, may provide insights into the biology of tumor angiogenesis and be used for diagnostic applications.

### Other Non-Primate Mammal Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20echistatin%20and%20%28animals%20not%20rodentia%20not%20primate%29)]

No publication is currently available.

### Non-Human Primate Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20echistatin%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20echistatin%20and%20human%20not%20rodentia)]

No publication is currently available.

## NIH Support

K08 HL03810, R01 HL48890, R01 HL65704

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
5 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
6 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
7 Battegay E.J. (1995). Angiogenesis: mechanistic insights, neovascular diseases, and therapeutic prospects. J Mol Med.
8 Folkman J. (2003). Fundamental concepts of the angiogenic process. Curr Mol Med.
9 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
10 Carmeliet P. (2003). Angiogenesis in health and disease. Nat Med.
11 Folkman J. (2003). Angiogenesis and proteins of the hemostatic system. J Thromb Haemost.
12 Carmeliet P. (2000). Mechanisms of angiogenesis and arteriogenesis. Nat Med.
13 Folkman J. (2004). Endogenous angiogenesis inhibitors. Apmis.
14 O'Reilly M.S., Holmgren L., Shing Y., Chen C., Rosenthal R.A., Cao Y., Moses M., Lane W.S., Sage E.H., Folkman J. (1994). Angiostatin: a circulating endothelial cell inhibitor that suppresses angiogenesis and tumor growth. Cold Spring Harb Symp Quant Biol.
15 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
16 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
17 Miller J.C., Pien H.H., Sahani D., Sorensen A.G., Thrall J.H. (2005). Imaging angiogenesis: applications and potential for drug development. J Natl Cancer Inst.
18 McLane M.A., Sanchez E.E., Wong A., Paquette-Straub C., Perez J.C. (2004). Disintegrins. Curr Drug Targets Cardiovasc Haematol Disord.
19 Leong-Poi H., Christiansen J., Klibanov A.L., Kaul S., Lindner J.R. (2003). Noninvasive assessment of angiogenesis by ultrasound and microbubbles targeted to alpha(v)-integrins. Circulation.
20 Ellegala D.B., Leong-Poi H., Carpenter J.E., Klibanov A.L., Kaul S., Shaffrey M.E., Sklenar J., Lindner J.R. (2003). Imaging tumor angiogenesis with contrast ultrasound and microbubbles targeted to alpha(v)beta3. Circulation.
21 Lindner J.R., Song J., Christiansen J., Klibanov A.L., Xu F., Ley K. (2001). Ultrasound assessment of inflammation and renal tissue injury with microbubbles targeted to P-selectin. Circulation.